# 1-O-(4-(2-[^18^F]Fluoroethyl-carbamoyloxymethyl)-2-nitrophenyl)-O-β-D-glucopyronuronate

Chemical name: | 1-O-(4-(2-[^18^F]Fluoroethyl-carbamoyloxymethyl)-2-nitrophenyl)-O-β-D-glucopyronuronate
Abbreviated name: | [^18^F]FEAnGA
Synonym:
Agent Category: | Compound
Target: | β-Glucuronidase (β-GUS; βG)
Target Category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | Yes
Studies: | - In vitro; - Rodents | Click on above structure for more information in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Glucuronidase&cmd=DetailsSearch)]

The β-glucuronidase (β-GUS; EC 3.2.1.31) is a lysosomal enzyme that is known to activate prodrugs (PDs) for the treatment of cancer. β-GUS has been used to track the path of gene delivery vehicles, and there is evidence that it can be used as a tumor marker (1). The primary function of the enzyme is to catalyze the hydrolysis of β-glucuronic acid residues from the cell-surface glycosaminoglycans for normal restructuring of the extracellular matrix (ECM) (2), and the enzyme is believed to participate in the processes of angiogenesis, cancer metastasis, and inflammation (3). Normal tissues have low levels of β-GUS in the ECM, but tissues under pathological stress, such as bacterial infection, fibrosis, and malignancy, show elevated levels of the enzyme (4). Intracellular β-GUS is released from necrotic cells, and its activity in these lesions has been used to activate anti-cancer PDs in situ to treat cancers (2). Chemotherapeutic anti-cancer drugs are generally nonselective and toxic to healthy cells; thus, they are of limited efficacy to the patient due to their side effects. The conversion of a toxic drug into a non-toxic PD that can be activated only under specific conditions (e.g., enzyme catalysis or chemical hydrolysis) would facilitate drug activation only in tissues that provide the specialized microenvironment and improve its concentration and efficacy at the desired location in the body (5, 6). For example, glucuronide PDs (drugs that are linked to a glucuronic acid moiety with or without a linker) have been shown to have superior anti-tumor activity compared with the parent drugs because the activated drugs are released from the PDs by the β-GUS activity in a site-specific manner (7, 8).

β-GUS activity varies among individuals, and its expression or accumulation in tumor tissues may change depending on the location in the body or the type of neoplasm (2, 9). Fluorescent or bioluminescent substrates were developed to determine the expression of β-GUS with optical imaging in various tissues of mice (1). However, this imaging modality is suitable for the detection of fluorescence or bioluminescence signals generated only in the superficial tissues of small animals such as rodents; the low depth of light penetration in tissues is a limitation for its application in large animals and humans (2, 4, 10). Imaging modalities such as positron emission tomography (PET) and single-photon emission computed tomography (SPECT), which use radionuclides to generate tracer signals, can be used to detect and determine the activity of enzymes such as the β-GUS because signals generated by radiolabeled probes can be detected even in deep tissues of the body (11). In general, PET imaging has a higher sensitivity than SPECT and has been used to investigate drug kinetics in preclinical and clinical settings (11). A ^124^I-labeled phenolphthalein glucuronide PD probe ([^124^I]-PTH-G) was developed and evaluated with microPET for the detection of xenograft tumors that express β-GUS in mice (9). Although [^124^I]-PTH-G was suitable for the detection of tumors in the rodents, biodistribution studies of the tracer in these animals revealed that, even at 20 h postinjection (p.i.), higher levels of the label could be detected in the liver, gallbladder, stomach, and intestines than in the tumors. Therefore, the investigators concluded that [^124^I]-PTH-G is probably unsuitable for the imaging of tumors that express β-GUS.

Antunes et al. synthesized 1-O-(4-(2-[^18^F]fluoroethyl-carbamoyloxymethyl)-2-nitrophenyl)-O-β-D-glucopyronuronate ([^18^F]-FEAnGA) as a PD in an effort to develop a probe that could be used with PET to detect and visualize β-GUS activity in tissues (4). The mechanism of in vitro or in vivo activation of [^18^F]-FEAnGA is described elsewhere (4). Briefly, the hydrolysis of [^18^F]-FEAnGA by β-GUS results in the production of glucuronic acid, 4-hydroxy-3-nitrobenzyl alcohol (HNBA; this is the spacer in the intact FEAnGA molecule, and the concentration of HNBA in the reaction mixture can be measured with ultraviolet (UV) spectroscopy at 402 nm after the FEAnGA has been hydrolysed), and 2-[^18^F]fluoroethylamine ([^18^F]-FEA). [^18^F]-FEA subsequently accumulates in the cells (attributed to passive diffusion into the cells) and is detected with PET imaging. [^18^F]-FEAnGA has been evaluated for the detection of tumors that expressed β-GUS (2, 4) and inflammation (2, 10) in mice.

### Related Resource Links

Other prodrug chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Prodrug+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Homo sapiens β-GUS protein and mRNA sequences (http://www.ncbi.nlm.nih.gov/nuccore/NM_000181.3)

Prodrug-related clinical trials (http://clinicaltrials.gov/ct2/results?term=prodrugs)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-FEAnGA%20synthesis&cmd=DetailsSearch)]

The synthesis of FEAnGA and its labeling with [^18^F]-fluoride have been described by Antunes et al. (4). The radiochemical yield (RCY) and radiochemical purity (RCP) of the labeled compound were reported to be 5%–20% (decay-corrected based on [^18^F]-fluoride) and 95%, respectively. The total time required for the synthesis and purification of the final labeled product was 150 min, and the specific activity of [^18^F]-FEAnGA was 5–10 GBq (135–270 μC)/μmol.

[^18^F]-FEA was synthesized for use in studies (4). The RCY of this radiochemical was 48 ± 9%. The RCP, specific activity, and stability of [^18^F]-FEA were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-FEAnGA%20in%20vitro&cmd=DetailsSearch)]

[^18^F]-FEAnGA was stable in phosphate-buffered saline (pH not reported) and rat plasma at 37°C for at least 1 h and 3 h, respectively, as determined with radio-thin-layer chromatography (radio-TLC) (4).

The lipophilicity (Log D) of [^18^F]-FEAnGA in an n-octanol/water mixture was determined to be −1.01 ± 0.03 and −1.61 ± 0.01 at pH 3 and pH 7.4, respectively (4). The lipophilicity of [^18^F]-FEA at pH 7.4 was determined to be −0.69 ± 0.02. This indicated that [^18^F]-FEAnGA was ~10-fold more hydrophilic than [^18^F]-FEA due to the presence of a glucuronic acid moiety in its structure (4).

The enzyme kinetics parameters for nonradioactive FEAnGA with Escherichia coli β-GUS and bovine liver β-GUS are presented in Table 1 and will not be discussed here.

Table 1: E. coli β-GUS and bovine liver β-GUS enzyme kinetic parameters with FEAnGA ( 4 )

β -GUS Enzyme | Substrate | K _ M _ (μM) | V _ max _ (μmol/min per mg) | k_cat_ (s−^1^) | k_cat_/K_M_ (10^6^/M−^1^ s−^1^)
E. coli | PNPG | 8.2 ± 1.6 | 1,366 ± 68 | 660 | 80.3
E. coli | FEAnGA | 7.1 ± 0.9 | 348 ± 24 | 134 | 24.6
Bovine liver β-GUS | PNPG | 34.0 ± 16.5 | 56.9 ± 23 | 19 | 0.6
Bovine liver β-GUS | FEAnGA | 5.7 ± 2.7 | 25.8 ± 9 | 10 | 1.8

PNPG, p-nitro-phenyl-β-D-glucuronide, a reference substrate for β-GUS; K_M_, Michaelis constant;

V_max_, velocity of the reaction; k_cat_, determines the catalytic formation of product under optimal reaction

conditions; k_cat_/K_M_, measure of the enzyme efficiency.

When C6 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CCL-107&Template=cellBiology) rat glioma cells were incubated with [^18^F]-FEAnGA in the presence of either E. coli β-GUS or bovine liver β-GUS (in growth medium containing 10% fetal bovine serum), 4- and 1.5-fold higher amounts of radioactivity were observed to be associated with the cells, respectively, compared with controls (4). In addition, when C6 cells were incubated with [^18^F]-FEA alone the amount of radioactivity associated with the cells was ~6-fold higher than the radioactivity associated with cells exposed to [^18^F]-FEAnGA without the β-GUS enzymes. The investigators ascribed the high uptake of radioactivity from [^18^F]-FEA by the C6 cells to passive diffusion of the label across the cell membrane (4). Under these incubation conditions, 99% and 37% of [^18^F]-FEAnGA was converted to [^18^F]-FEA by the E. coli β-GUS and bovine liver β-GUS enzymes, respectively, as determined with radio-TLC of the cell growth medium.

The uptake of radioactivity from [^18^F]-FEAnGA and [^18^F]-FEA was also studied in CT26 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2638&Template=cellBiology) cells (wild-type mouse colon adenocarcinoma cells) and CT26mβGUS cells (CT26 cells that are engineered to express β-GUS as an anchored enzyme on the outer surface of the cell membrane) (4). With [^18^F]-FEA, a 14-fold higher amount of radioactivity accumulated in the control CT26 cells than with [^18^F]-FEAnGA. Incubation of CT26 cells (controls) and the CT26mβGUS cells with [^18^F]-FEAnGA showed that the latter cells had a 3-fold higher amount of radioactivity associated with the cells compared with the control cells. Radio-TLC of the growth medium of the CT26mβGUS cells showed that 20% of the [^18^F]-FEAnGA was converted to [^18^F]-FEA by the β-GUS anchored on the membrane surface of these cells (4).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-FEAnGA%20rodentia&cmd=DetailsSearch)]

A preliminary study was performed in two mice bearing CT26 and CT26βGUS cell tumors on the right and left shoulders, respectively, to evaluate the use of [^18^F]-FEAnGA for the detection of β-GUS expression with PET (4). The animals were injected with either [^18^F]-FEAnGA (4.4 MBq (118.8 μCi)) or [^18^F]-FEA (4.2 MBq (113.4 μCi)) through the penile vein, and a microPET scan was acquired for 60 min. At 1 h p.i., PET images of the animal injected with [^18^F]-FEAnGA showed a 2-fold higher uptake of radioactivity in the CT26βGUS cell tumor compared with the CT26 cell control tumor. The increased uptake of radioactivity by the CT26βGUS tumor was attributed to the production of [^18^F]-FEA from [^18^F]-FEAnGA by the β-GUS on the surface of the CT26βGUS cells (4). The animals injected with [^18^F]-FEA did not show any accumulation of radioactivity in the CT26βGUS cell tumor. No blocking studies were reported. From this preliminary study, the investigators concluded that [^18^F]-FEAnGA may be used as a tracer to visualize tumors that express the β-GUS enzyme in rodents (4).

The ex vivo biodistribution of [^18^F]-FEAnGA was investigated in healthy anesthetized Wistar rats (n = 5 animals) injected with 5.04 ± 1.80 MBq (136.08 ± 48.6 μCi) of the radiochemical through the penile vein (2). At 60 min p.i., very low radioactivity uptake was observed in the major organs of the animals. The kidneys showed an uptake of 0.53 ± 0.24 standardized uptake values (SUV), and the liver showed an uptake of 0.15 ± 0.04 SUV, indicating that the tracer was cleared rapidly from the system through the renal pathway.

The use of [^18^F]-FEAnGA with PET was evaluated for the detection of C6 cell tumors or muscular inflammation (induced with turpentine) in Wistar rats (n = 8 animals) (2). Two microPET scans were acquired from each animal after [^18^F]-FEAnGA injection as described above. The first scan was performed to detect small (<1.5 cm^3^) and large (>1.5 cm^3^) tumors at 8 days after inoculation of the C6 cells to induce the tumors. The second PET scan was performed for the detection of the tumor and inflammation at 13 days after the C6 injection. Images obtained from the first PET scan showed that there was a uniform distribution of radioactivity from [^18^F]-FEAnGA in the small tumors; however, the large tumors showed a high uptake of label only in the viable outer periphery of the lesions, whereas the non-viable parts of the large tumors had a low accumulation of the tracer. Time-activity curves of the tumors showed that the small tumors had peak accumulation of radioactivity at 1.5 min p.i. with a tracer half-life of 12 ± 3 min. The half-life of radioactivity in the viable parts of the large tumors was reported to be 24 ± 13 min, and the area under the curve (AUC) for these lesions was 1.7-fold greater than that of the small tumors (P = 0.05). The PET scan at 13 days after inoculation of the C6 cells showed that the accumulation of radioactivity in the inflamed muscle (0.07 ± 0.05 SUV) was significantly higher than that observed in the normal muscle (0.04 ± 0.03 SUV; P < 0.05). From these studies, the investigators concluded that [^18^F]-FEAnGA can be used to detect and understand the activity of β-GUS in cancerous tumors and inflamed tissues in rodents (2).

The use of [^18^F]-FEAnGA with PET was evaluated in a rat model of herpes encephalitis for the detection of β-GUS activity released in the tissue during neuroinflammation (10). Male Wistar rats were infected with herpes simplex virus-1 (HSV-1) to induce herpes encephalitis in the animals (n = 8 rats; as controls, n = 4 rats), and microPET scans were acquired from the rodents after intravenous penile injection of [^18^F]-FEAnGA as described above (10). A low uptake of radioactivity was observed in the brains of the infected and the control animals. The AUC (10–60 min p.i.) for whole brains of the HSV-1–infected animals was 2-fold higher (P = 0.05) than that of the control rats (AUC = 5 ± 1). Brain homogenates of the HSV-1–infected rats showed 3.4-fold higher activity of β-GUS compared with the enzyme activity in the brain homogenates of control animals (10). From this study, the investigators concluded that, although there was a low uptake of label from [^18^F]-FEAnGA in the brain, this tracer could be used to detect increased β-GUS activity in the organ due to neuroinflammation (10).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-FEAnGA%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-FEAnGA%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-FEAnGA%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Cheng T.C., Roffler S.R., Tzou S.C., Chuang K.H., Su Y.C., Chuang C.H., Kao C.H., Chen C.S., Harn I.H., Liu K.Y., Cheng T.L., Leu Y.L. (2012). An activity-based near-infrared glucuronide trapping probe for imaging beta-glucuronidase expression in deep tissues. J Am Chem Soc.
2 Antunes I.F., Haisma H.J., Elsinga P.H., van Waarde A., Willemsen A.T., Dierckx R.A., de Vries E.F. (2012). In Vivo Evaluation Of 1-o-(4-(2-fluoroethyl-carbamoyloxymethyl)-2-nitrophenyl)-o-beta-d-glucopyronurona te: A Positron Emission Tomographic Tracer For Imaging beta-glucuronidase Activity In A Tumor/inflammation Rodent Model. Mol Imaging.
3 Gandhi N.S., Freeman C., Parish C.R., Mancera R.L. (2012). Computational analyses of the catalytic and heparin-binding sites and their interactions with glycosaminoglycans in glycoside hydrolase family 79 endo-beta-D-glucuronidase (heparanase). Glycobiology.
4 Antunes I.F., Haisma H.J., Elsinga P.H., Dierckx R.A., de Vries E.F. (2010). Synthesis and evaluation of [18F]-FEAnGA as a PET Tracer for beta-glucuronidase activity. Bioconjug Chem.
5 Antunes I.F., Haisma H.J., de Vries E.F. (2008). Tumor-specific activation of prodrugs: is there a role for nuclear medicine?. Nucl Med Commun.
6 Huttunen K.M., Raunio H., Rautio J. (2011). Prodrugs--from serendipity to rational design. Pharmacol Rev.
7 Thomas M., Clarhaut J., Tranoy-Opalinski I., Gesson J.P., Roche J., Papot S. (2008). Synthesis and biological evaluation of glucuronide prodrugs of the histone deacetylase inhibitor CI-994 for application in selective cancer chemotherapy. Bioorg Med Chem.
8 Renoux B., Legigan T., Bensalma S., Chadeneau C., Muller J.M., Papot S. (2011). A new cyclopamine glucuronide prodrug with improved kinetics of drug release. Org Biomol Chem.
9 Tzou S.C., Roffler S., Chuang K.H., Yeh H.P., Kao C.H., Su Y.C., Cheng C.M., Tseng W.L., Shiea J., Harm I.H., Cheng K.W., Chen B.M., Hwang J.J., Cheng T.L., Wang H.E. (2009). Micro-PET imaging of beta-glucuronidase activity by the hydrophobic conversion of a glucuronide probe. Radiology.
10 Antunes I.F., Doorduin J., Haisma H.J., Elsinga P.H., van Waarde A., Willemsen A.T., Dierckx R.A., de Vries E.F. (2012). 18F-FEAnGA for PET of beta-Glucuronidase Activity in Neuroinflammation. J Nucl Med.
11 Willmann J.K., van Bruggen N., Dinkelborg L.M., Gambhir S.S. (2008). Molecular imaging in drug development. Nat Rev Drug Discov.